# ^18^F-Labeled poly(L-lactic acid)-block-poly(sarcosine) lactosome, a polymer micelle

Chemical name: | ^18^F-Labeled poly(L-lactic acid)-block-poly(sarcosine) lactosome, a polymer micelle
Abbreviated name: | [^18^F]-Lactosome
Synonym:
Agent Category: | Compound
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Radiolabeled%20nanocarriers&cmd=DetailsSearch)]

[^18^F]Fluoro-D-glucose ([^18^F]FDG) (an analog of glucose that is transported through the glucose transporter) is the most common radiotracer used with positron emission tomography (PET)/computed tomography for the clinical detection, diagnosis, staging, and monitoring of cancerous tumors (1). Transformed cells have a high metabolic rate and tend to accumulate [^18^F]FDG because this labeled compound is not metabolized by the cells. The accumulation of this labeled compound facilitates the noninvasive imaging of tumors with PET. However, the use of [^18^F]FDG to detect cancerous lesions has several limitations. For example, this technique may not detect neoplastic tumors that grow slowly and exhibit a very small increase in glucose consumption, such as those of the thyroid or neuroendocrine tissues. In addition, PET imaging may not distinguish a tumor from the background signal in organs that have a high glucose metabolism, such as the brain and the liver. Furthermore, [^18^F]FDG is not able to differentiate inflamed tissues from neoplastic tumors because both of these pathologies exhibit a characteristic high glucose metabolism (2). As a consequence, there is much interest to develop and evaluate alternative radiopharmaceuticals, including nanoparticles, that can be used for the PET imaging of tumors (3).

Nanoparticles (NP) can range from 1 nm to 100 nm in diameter, may have an inorganic (e.g., iron oxide and gold), lipid (e.g., liposomes), or polymeric (e.g., poly(L-lactic acid)) structure, and have been investigated for a wide range of medical applications, including preclinical and clinical imaging as described in detail elsewhere (4). Polymeric NPs are biocompatible and biodegradable, and they show greater in vivo stability compared with inorganic or lipid nanoparticles. Therefore, polymeric NPs are considered to be well suited for the development of molecular imaging probes (3). It has been shown that a near-infrared fluorescence (NIRF) dye-labeled poly(L-lactic acid)-block-poly(sarcosine) amphiphilic polydepsipeptides, designated as a lactosome, can be used to visualize solid tumors with NIRF imaging because NIRF-labeled NPs accumulate in cancerous lesions due to the enhanced permeability and retention effect (5). Lactosomes are reported to have a long circulation time because their surface is covered with hydrophilic poly(sarcosine) chains; because they have a narrow size distribution range of ~35 nm, these NPs are not entrapped by the reticuloendothelial system. On the basis of the NIRF-lactosome study, it was hypothesized that ^18^F-labeled lactosomes ([^18^F]-lactosomes) can probably be used with PET for the detection of solid tumors (3).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Labeled+nanoparticles+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Nanoparticles&Search=Search) related to nanoparticles

Enhanced permeation and retention effect [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=enhanced%20permeation%20retention%20effect&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis and ^18^F labeling of lactosomes has been described in detail by Yamamoto et al. (3). Each synthesis reaction was reported to produce 222–420 MBq (6–11.35 mCi) [^18^F]-lactosomes, with a radiochemical yield of >95% and a radiochemical purity of >95% as determined with Sephacryl S-100 HR chromatography. The specific activity of the purified [^18^F]-Lactosomes preparation was not reported. The total time required to synthesize and purify the labeled lactosomes was 200–220 min (3).

Indocyanine green–labeled lactosomes (NIRF-lactosomes) were also prepared for use as controls in the PET imaging studies (3). Purity of the NIRF-lactosomes was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Lactosome%20In%20Vitro%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Lactosome%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-lactosomes was investigated in mice bearing HeLa cell (http://atcc.org/Products/All/CCL-2.2.aspx) tumors (3). The animals (n = 3 mice/time point) were injected with 10 MBq (0.27 mCi) [^18^F]-lactosomes per mouse through the tail vein, and the rodents were euthanized at predetermined time points ranging from 10 min postinjection (p.i.) to 6 h p.i. All organs of interest, including tumors, were removed from the animals, and the amount or radioactivity accumulated in the various tissues was determined. Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). At 10 min p.i., maximum radioactivity was observed in the blood (~45% ID/g), followed by lungs (~27% ID/g), heart (~10% ID/g), and spleen (~5% ID/g). By 6 h p.i., the amount of radioactivity in the blood, lungs, and heart was reduced to ~25% ID/g, 12% ID/g, and 5% ID/g, respectively, but in the spleen it increased to ~10% ID/g. The liver and kidneys each showed an uptake of ~5% ID/g at 10 min p.i.; by 6 h p.i., the amount of label in these organs was ~5% ID/g and ~10% ID/g, respectively. The tumors showed an uptake of ~1.5% at 10 min p.i., and the uptake increased to ~2.7% ID/g by 6 h p.i. The tumor/blood and tumor/muscle uptake ratios increased from 0.02 ± 0.00 and 1.29 ± 0.23, respectively, at 10 min p.i. to 0.09 ± 0.00 and 2.66 ± 0.36, respectively, at 6 h p.i. The tumor/digestive tract and tumor/brain uptake ratios at 6 h p.i. were reported to be 2.8 and 4.9, respectively.

For PET imaging, the tumor-bearing mice (n = 3 animals/time point; under anesthesia) were coinjected with 5.0–13.6 MBq (0.135–0.367 mCi) [^18^F]-lactosomes and NIRF-lactosomes, and whole-body PET scans of the animals were acquired at various time points (3). At 6 h p.i., accumulated radioactivity was clearly visible in the heart, bladder, and tumors. No tracer was visible in the brain, muscles, or bone at 6 h p.i., and the tumor/muscle ratio was calculated to be 2.2 ± 0.1 at 6 h p.i. NIRF images were acquired from the same animals immediately after completion of the PET scans (3). The tumors were clearly visible in the NIRF images at 6 h p.i., and the tumor/muscle ratio was determined to be 1.5 ± 0.3.

From these studies, the investigators concluded that [^18^F]-lactosomes were probably suitable for the PET imaging of tumors in mice (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Lactosome%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Lactosome%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bactosome%20human%20studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Tomasi G., Rosso L. (2012). PET imaging: implications for the future of therapy monitoring with PET/CT in oncology. Curr Opin Pharmacol.
2 Nanni C., Fantini L., Nicolini S., Fanti S. (2010). Non FDG PET. Clin Radiol.
3 Yamamoto F., Yamahara R., Makino A., Kurihara K., Tsukada H., Hara E., Hara I., Kizaka-Kondoh S., Ohkubo Y., Ozeki E., Kimura S. (2013). Radiosynthesis and initial evaluation of (18)F labeled nanocarrier composed of poly(L-lactic acid)-block-poly(sarcosine) amphiphilic polydepsipeptide. Nucl Med Biol.
4 Liu Y., Welch M.J. (2012). Nanoparticles labeled with positron emitting nuclides: advantages, methods, and applications. Bioconjug Chem.
5 Makino A., Kizaka-Kondoh S., Yamahara R., Hara I., Kanzaki T., Ozeki E., Hiraoka M., Kimura S. (2009). Near-infrared fluorescence tumor imaging using nanocarrier composed of poly(L-lactic acid)-block-poly(sarcosine) amphiphilic polydepsipeptide. Biomaterials.